# IRDye 800CW-Epidermal growth factor

Chemical name: | IRDye 800CW-Epidermal growth factor
Abbreviated name: | IRDye 800CW-EGF
Synonym:
Agent category: | Polypeptide
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20and%20EGF)]

Epidermal growth factor (EGF) is a 53–amino acid cytokine (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, which include EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasm tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (11-13). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, which provides a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody against the extracellular domain of recombinant HER2 (14), and C225, an anti-EGFR chimeric monoclonal antibody, have been labeled as ^111^In-trastuzumab (15-17) and ^99m^Tc-EC-C225 (C225 is also known as cetuximab) (18, 19), respectively, for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). However, antibodies that are approximately 25-fold larger than EGF may not be easily transported to cells within solid tumors. ^111^In- and ^68^Ga-labeled trastuzumab F(ab) antibody fragments as well as ^111^In-EGF and ^99m^Tc-HYNIC-EGF have been used to partially overcome this permeability barrier (20, 21). EGF has also been successfully coupled with Cy5.5 NIR dye (22) and IRDye 800CW (23) for optical imaging of EGFR density in tumors in mice using non-radioactive materials.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20synthesis)]

Commercially available IRDye 800CW-N-hydroxysuccinimide ester (LI-COR, Lincoln, NE) was used to conjugate EGF to form IRDye 800CW-EGF, which was purified by dialysis (23). The molar ratio of IRDye 800CW to EGF and yield were not reported. IRDye 800CW (molecular weight, 962 Da) has an extinction coefficient of 237,000 M^-1^cm^-1^ and a quantum yield of 0.12, with a maximum excitation wavelength of 783 nm and a maximum emission wavelength of 801 nm in fetal bovine serum.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20in%20vitro)]

Kovar et al. (23) performed cell-binding assays with IRDye 800CW-EGF using human prostate cancer cell lines PC3M-LN4 (EGFR-positive, metastatic) and 22Rv1 (EGFR-positive, non-metastatic). Incubation of IRDye 800CW-EGF (1–70 nM) for 2 min at 37°C resulted in high fluorescence intensity in both cell lines in a dose-dependent manner. On the other hand, IRDye 800CW binding in both cell types was negligible. Binding of IRDye 800CW-EGF was completely blocked by C225 (100 μg) and EGF (1 μM) with inhibition constant (IC_50_) values of 10 μg and 0.1 μM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20rodentia)]

Kovar et al. (23) studied the accumulation of IRDye 800CW-EGF using a whole-body fluorescence detection system in nude mice bearing PC3M-LN4 tumors. IRDye 800CW-EGF (1 nmol/mouse) was injected intravenously into mice that showed distinct fluorescence signals in the tumors and lymph nodes at 72–96 h after injection. The fluorescence intensity started to decrease after 96 h. Pretreatment with C225 (13 nmol/mouse 60 min before IRDye 800CW-EGF injection) inhibited the IRDye 800CW-EGF binding in the tumors and lymph nodes by 34–46% (nonspecific IgG antibody pretreatment was not performed). Other experiments showed that the accumulation of IRDye 800CW-EGF was distinctly higher in the 22Rv1 tumors than in the PC3M-LN4 tumors as the tumors grew in size. However, all mice with PC3M-LN4 tumors (n = 4) were node-positive, and all 22Rv1 tumor-bearing mice (n = 4) were node-negative, which confirmed that PC3M-LN4 is metastatic and 22Rv1 is non-metastatic.

Adams et al. (24) performed in vivo whole-body fluorescence imaging of IRDye 800CW-EGF (1 nmol) in nude mice (n = 5) bearing EGFR-positive MDA-MB-468 and EGFR-negative MDA-MB-435 human breast cancer cells at 24 h after injection. Accumulation into MDA-MB-468 tumors was higher than MDA-MB-435 tumors. Pretreatment with C225 (13 nmol/mouse 24 h before IRDye 800CW-EGF injection) inhibited the IRDye 800CW-EGF binding in the tumors by ~50%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=800CW%20EGF%20and%20human)]

No publication is currently available.

## NIH Support

R01 CA106584-01A1, R01 CA106584-02, R01 EB003132, R01 EB005173

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
12 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
13 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
14 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
15 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
16 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
17 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
18 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
19 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
20 Josephson L., Kircher M.F., Mahmood U., Tang Y., Weissleder R. (2002). Near-infrared fluorescent nanoparticles as combined MR/optical imaging probes. Bioconjug Chem.
21 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
22 Ke S., Wen X., Gurfinkel M., Charnsangavej C., Wallace S., Sevick-Muraca E.M., Li C. (2003). Near-infrared optical imaging of epidermal growth factor receptor in breast cancer xenografts. Cancer Res.
23 Kovar J.L., Johnson M.A., Volcheck W.M., Chen J., Simpson M.A. (2006). Hyaluronidase expression induces prostate tumor metastasis in an orthotopic mouse model. Am J Pathol.
24 Adams K.E., Ke S., Kwon S., Liang F., Fan Z., Lu Y., Hirschi K., Mawad M.E., Barry M.A., Sevick-Muraca E.M. (2007). Comparison of visible and near-infrared wavelength-excitable fluorescent dyes for molecular imaging of cancer. J Biomed Opt.